# [^177^Lu]-Labeled [(R)-2-amino-3-(4-isothiocyanatophenyl)propyl]-trans-(S,S)-cyclohexane-1,2-diamine-pentaacetic acid (CHX-A″-DTPA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII)

Chemical name: | [^177^Lu]-Labeled [(R)-2-amino-3-(4-isothiocyanatophenyl)propyl]-trans-(S,S)-cyclohexane-1,2-diamine-pentaacetic acid (CHX-A″-DTPA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII)
Abbreviated name: | [^177^Lu]CHX-A''-DTPA-L8A4
Synonym:
Agent Category: | Monoclonal antibody
Target: | Epidermal growth factor receptor variant III (EGFRvIII)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography; gamma planar imaging
Source of signal / contrast: | ^177^Lu
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ch806&cmd=DetailsSearch)]

The biological characteristics, activating ligands, functions, and signal transduction pathways of the various transmembrane epidermal growth factor receptors (EGFRs) are described elsewhere (1-3). The EGFRs are known to regulate the growth, survival, differentiation, and migration of cells through the activation of an associated intracellular tyrosine kinase (TK) signaling pathway, and they are overexpressed in many malignant epithelial tumors (2, 3). Overexpression of the EGFR in tumors has been attributed to cellular amplification of the receptor gene, and this phenomenon may result in the production of a mutated receptor in the cell (2, 4). In addition, overexpression of the EGFR in tumors usually indicates a poor clinical prognosis for a cancer patient (4). The most common mutation observed in the receptor is the deletion of an extracellular domain segment of the EGFR, including the ligand-binding region, and this generates a variant known as EGFRvIII or de2-7 EGFR (2, 4). The generation, structure, functions, and role of EGFRvIII in tumor malignancy was reviewed by Gan et al. (5). Although EGFRvIII is nonresponsive to a ligand due to the absence of a ligand-binding site, it is constitutively active with a constantly operating downstream TK signal transduction pathway that appears to promote the development of a neoplastic phenotype, particularly for glioblastoma and to some extent for other cancers such as those of the prostate and the breast (2, 6).

Because the EGFR promotes and helps maintain transformed cells, several anti-EGFR antibodies (http://google2.fda.gov/search?q=anti-EGFR+antibodies+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=6) that inhibit the activity of this receptor and small molecule drugs (http://google2.fda.gov/search?q=EGFR+Tyrosine+kinase+inhibitor&spell=1&client=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&ie=UTF-8&site=FDAgov&access=p) that block the downstream TK signaling pathway were developed and have been approved by the United States Food and Drug Administration for the treatment of certain cancers (2). The antibodies are designed to target the extracellular domain of the receptor, block ligand binding, and inhibit activation of the TK signal transduction pathway, which leads to downregulation of the EGFR on the cell surface. However, because EGFRvIII lacks the ligand-binding region on the extracellular domain, these antibodies cannot obstruct the constitutive mutant receptor activity (2). Hence, a monoclonal antibody (1), designated mAb806 and specifically targets the EGFRvIII, was generated and has been characterized in preclinical studies (7, 8). Subsequently, a chimeric form of the mAb (chAb), designated ch806, was developed and evaluated in a phase I clinical trial involving patients with cancerous tumors that overexpressed the EGFRvIII. Results from this trial indicated that ch806 can be a suitable biotherapeutic agent to treat cancers (4). Various studies performed with mAb806 or ch806 are described in separate chapters of MICAD (http://www.ncbi.nlm.nih.gov/books/?term=ch806%20AND%20micad%5Bbook%5D).

Studies are also in progress with another anti-EGFRvIII mAb, L8A4, to develop a radioimmunotherapeutic (RIT) agent for the treatment of cancer (9, 10). In a recent study, the use of acyclic ([(R)-2-amino-3-(4-isothiocyanatophenyl)propyl]-trans-(S,S)-cyclohexane-1,2-diamine-pentaacetic acid (CHX-A''-DTPA) and 2-(4-isothiocyanatobenzyl)-6-methyldiethylene-triaminepentaacetic acid (1B4M-DTPA) as well as the macrocyclic ligands (S)-2-(4-isothiocyanatobenzyl)-1,4,7,10-tetraazacyclododecane-tetraacetic acid (C-DOTA) and α-(5-isothiocyanato-2-methoxyphenyl)-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (MeO-DOTA) was evaluated for the labeling of L8A4 with ^177^Lu, which was considered suitable to generate an RIT agent against cancer (10). The characteristics of the various ^177^Lu-labeled conjugates of L8A4 ([^177^Lu]-CHX-A''-DTPA-L8A4, [^177^Lu]-1B4M-DTPA-L8A4, [^177^Lu]-C-DOTA-L8A4, and [^177^Lu]-MeO-DOTA-L8A4) were compared to the characteristics of L8A4 labeled with N-succinimidyl 4-guanidinomethyl-3-[^125^I]iodobenzoate ([^125^I]SGMIB-L8A4) under in vitro (9) and in vivo (10) conditions.

This chapter describes results obtained from the in vitro and the biodistribution studies performed with [^177^Lu]-CHX-A''-DTPA-L8A4 in athymic mice bearing subcutaneous U87MG.∆EGFR cell glioma xenograft tumors. Results obtained with [^125^I]SGMIB-L8A4, [^177^Lu]-1B4M-DTPA-L8A4, [^177^Lu]-C-DOTA-L8A4, and [^177^Lu]-MeO-DOTA-L8A4 are presented in separate chapters of MICAD (www.micad.nih.gov) (11-14).

### Other Sources of Information

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_005228.3) of human EGFR variant 1

EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim/131550) (Online Mendelian Inheritance in Man)

EGFR signaling pathways (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=200086&source=NATURE&what=graphic&jpg=on) (NCI-Nature Pathways Interaction Database)

Anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-EGFR%20antibodies&cmd=DetailsSearch) in PubMed

EGFR tyrosine kinase inhibitors (http://www.ncbi.nlm.nih.gov/pubmed?term=egfr%20tyrosine%20kinase%20inhibitors&cmd=DetailsSearch) in PubMed

Chapters on anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD

Other chapters on anti-EGFRvIII antibodies (http://www.ncbi.nlm.nih.gov/books/?term=EGFRvIII%20AND%20micad%5Bbook%5D) in MICAD

Clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFRvIII+) with EGFRvIII as a target

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Synthesis%20of%20L8A4%20antibody&cmd=DetailsSearch)]

The preparation, purification, characterization, conjugation with CHX-A''-DTPA, and radiolabeling of CHX-A''-DTPA-L8A4 with ^177^Lu are discussed by Hens et al. (10). The production of [^125^I]SGMIB-L8A4 (labeled with ^125^I using N-succinimidyl 4-guanidinomethyl-3-[^125^I]iodobenzoate ([^125^I]SGMIB)) is also described by Hens et al. (10). The radiochemical yield (RCY) of [^177^Lu]-CHX-A''-DTPA-L8A4 was 76%. The RCY of [^125^I]SGMIB-L8A4 and the purity of the two labeled mAbs was not reported. The specific activity of [^177^Lu]-CHX-A''-DTPA-L8A4 was reported to be 0.092 MBq/6.6 pmol (2.5 μCi/6.6 pmol) and that of [^125^I]SGMIB-L8A4 varied from 0.111–0.185 MBq/6.6 pmol (3–5 μCi/6.6 pmol) to 0.026–0.118 MBq/6.6 pmol (0.7–3.2 μCi/6.6 pmol). The two labeled mAbs were shown to elute as a single peak with L8A4 and had a similar retention time as the native mAb when analyzed with a size-exclusion column using high performance liquid chromatography. Each mAb molecule was determined to bear 0.3 moieties of CHX-A''-DTPA (9, 10).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20in%20vitro%20studies&cmd=DetailsSearch)]

Using a magnetic bead assay, the immunoreactive fraction of [^177^Lu]-CHX-A''-DTPA-L8A4 was determined to be 60% compared to between 60% to 71% for [^125^I]SGMIB-L8A4 (9). A cell internalization assay with U87MG.∆EGFR cells showed that internalization of [^177^Lu]-CHX-A''-DTPA-L8A4 continued to increase for at least 24 h (was ~35% at this time point). With the ^125^I-labeled mAb the internalization of radioactivity peaked to ~10% of the original cell-bound radioactivity at 1 h after exposure and was reduced to ~1% of the original value by 24 h after exposure.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20rodentia&cmd=DetailsSearch)]

To investigate the biodistribution of [^177^Lu]-CHX-A''-DTPA-L8A4 and compared it to that of [^125^I]SGMIB-L8A4, athymic mice (n = 5 animals/group) bearing subcutaneous U87MG.∆EGFR cell glioma xenograft tumors were injected with a mixture of the two labeled mAbs as described by Hens et al. (10). The rodents were euthanized at 1, 4, and 8 days postinjection (p.i.) of the labeled mAbs and all major organs were harvested from the animals. Radioactivity incorporated in the various organs was counted using a dual-channel automated gamma counter and the data was presented as percent of injected dose per gram tissue (% ID/g). With [^177^Lu]-CHX-A''-DTPA-L8A4 the amount of radioactivity in the blood was 15.18 ± 3.30% ID/g at 1 day p.i. and this was reduced to 0.99 ± 0.71% ID/g by 8 days p.i. At 1 day p.i., the liver, kidneys, spleen, lungs and bone exhibited accumulation of between 8.53 ± 1.86% ID/g (liver) and 5.98 ± 1.86% ID/g (spleen) and the by 8 days p.i. amount of label in all these organs, except the bone, decreased to between 0.56 ± 0.23% ID/g (lungs) and 4.45 ± 0.87% ID/g (Liver). During this period the incorporation of radioactivity in the bone increased from 5.95 ± 1.27% ID/g at 1 day p.i. to 7.56 ± 1.88% ID/g at 8 days p.i. This phenomenon was attributed to the bone seeking characteristic of unchelated ^177^Lu indicating that [^177^Lu]-CHX-A''-DTPA-L8A4 may not be suitable detection agent for EGFRvIII expressing tumors. The amount of tracer accumulated in the muscles was 1.30 ± 0.44% Id/g at 1 day p.i. and was reduced to 0.19 ± 0.05% ID/g by 8 days p.i. The amount of radioactivity accumulated in the tumor was 36.28 ± 6.60% ID/g at 1 day p.i. and decreased to 8.67 ± 3.42% ID/g by 8 days p.i. The tumor/normal tissue ratios for liver, kidneys, spleen, brain, and bone were reported to be approximately 4, 6, 4, 95, and 6, respectively, at 1 day p.i. and approximately 2, 5, 2, 200 and 2, respectively at 8 days p.i.

With [^125^I]SGMIB-L8A4 the amount of radioactivity in the blood at 1 day p.i. was 18.78 ± 2.24% ID/g and decreased to 1.29 ± 0.87% ID/g by 8 days p.i. At 1 day p.i., the liver, kidneys, spleen, and lungs exhibited accumulation between 5% and 7% ID/g and the amount of label in all these organs decreased to ~0.5% ID/g by 8 days p.i. The amount of tracer accumulated in the muscles and bones was ~1.5 and ~3.5% ID/g, respectively, at 1 day p.i.; by 8 days p.i., accumulation decreased to ~0.15% ID/g and ~0.33% ID/g, respectively, in these tissues. The tumor had a radioactivity accumulation of 21.64 ± 4.53% ID/g at 1 day p.i., which decreased to 2.86 ± 0.98% ID/g by 8 days p.i. The tumor/normal tissue ratios for liver, kidneys, spleen, brain, and bone were reported to be approximately 6, 8, 6, 60, and 10, respectively, at 1 day p.i. and approximately 7, 8, 7, 60 and 6, respectively, at 8 days p.i.

Table 1: Summary of tumor/normal tissue radioactivity uptake ratios for various organs obtained with [ ^ 125 ^ I]SGMIB-L8A4 and [ ^ 177 ^ Lu]CHX-A”-DTPA-L8A4. Data obtained from Fig. 3 in Hens et. al. ( 10 ).

Conjugated mAb | Liver | | Kidney | | Spleen | | Brain | | Bone
Conjugated mAb | Time after labeled mAb injection
Conjugated mAb | 1 day | 8 days | 1 day | 8 days | 1 day | 8 days | 1 day | 8 days | 1 day | 8 days
Conjugated mAb | Tumor-to-normal tissue ratio
[ ^ 125 ^ I]SGMIB-L8A4 | 6 | 7 | 8 | 8 | 6 | 7 | 60 | 60 | 10 | 6
[ ^ 177 ^ Lu]CHX-A”-DTPA-L8A4 | 4 | 2 | 6 | 5 | 4 | 2 | 95 | 200 | 6 | 2

Based on the results presented in Table 1 [^125^I]SGMIB-L8A4 appeared to be superior to [^177^Lu]-CHX-A''-DTPA-L8A4 for the detection of EGFRvIII overexpressing tumors in rodents because it had higher tumor-to-normal tissue ratios compared to the ^177^Lu-labeled mAb during the entire duration of the experiment (10).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

These studies were supported by National Institutes of Health grants NS20023 and CA42324.

## References

1 Hasselbalch B., Lassen U., Poulsen H.S., Stockhausen M.T. (2010). Cetuximab insufficiently inhibits glioma cell growth due to persistent EGFR downstream signaling. Cancer Invest.
2 Pines G., Kostler W.J., Yarden Y. (2010). Oncogenic mutant forms of EGFR: lessons in signal transduction and targets for cancer therapy. FEBS Lett.
3 Spector N.L., Blackwell K.L. (2009). Understanding the mechanisms behind trastuzumab therapy for human epidermal growth factor receptor 2-positive breast cancer. J Clin Oncol.
4 Scott A.M., Lee F.T., Tebbutt N., Herbertson R., Gill S.S., Liu Z., Skrinos E., Murone C., Saunder T.H., Chappell B., Papenfuss A.T., Poon A.M., Hopkins W., Smyth F.E., MacGregor D., Cher L.M., Jungbluth A.A., Ritter G., Brechbiel M.W., Murphy R., Burgess A.W., Hoffman E.W., Johns T.G., Old L.J. (2007). A phase I clinical trial with monoclonal antibody ch806 targeting transitional state and mutant epidermal growth factor receptors. Proc Natl Acad Sci U S A.
5 Gan H.K., Kaye A.H., Luwor R.B. (2009). The EGFRvIII variant in glioblastoma multiforme. J Clin Neurosci.
6 Lee F.T., O'Keefe G.J., Gan H.K., Mountain A.J., Jones G.R., Saunder T.H., Sagona J., Rigopoulos A., Smyth F.E., Johns T.G., Govindan S.V., Goldenberg D.M., Old L.J., Scott A.M. (2010). Immuno-PET quantitation of de2-7 epidermal growth factor receptor expression in glioma using 124I-IMP-R4-labeled antibody ch806. J Nucl Med.
7 Jungbluth A.A., Stockert E., Huang H.J., Collins V.P., Coplan K., Iversen K., Kolb D., Johns T.J., Scott A.M., Gullick W.J., Ritter G., Cohen L., Scanlan M.J., Cavenee W.K., Old L.J. (2003). A monoclonal antibody recognizing human cancers with amplification/overexpression of the human epidermal growth factor receptor. Proc Natl Acad Sci U S A.
8 Perera R.M., Zoncu R., Johns T.G., Pypaert M., Lee F.T., Mellman I., Old L.J., Toomre D.K., Scott A.M. (2007). Internalization, intracellular trafficking, and biodistribution of monoclonal antibody 806: a novel anti-epidermal growth factor receptor antibody. Neoplasia.
9 Hens M., Vaidyanathan G., Welsh P., Zalutsky M.R. (2009). Labeling internalizing anti-epidermal growth factor receptor variant III monoclonal antibody with (177)Lu: in vitro comparison of acyclic and macrocyclic ligands. Nucl Med Biol.
10 Hens M., Vaidyanathan G., Zhao X.G., Bigner D.D., Zalutsky M.R. (2010). Anti-EGFRvIII monoclonal antibody armed with 177Lu: in vivo comparison of macrocyclic and acyclic ligands. Nucl Med Biol.
11 Chopra, A., [125I]-Labeled monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
12 Chopra, A., 177Lu-Labeled [(R)-2-amino-3-(4-isothiocyanatophenyl)propyl]-trans-(S,S)-cyclohexane-1,2-diamine-pentaacetic acid (CHX-A″-DTPA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
13 Chopra, A., 177Lu-Labeled (S-2-(4-isothiocyanatobenzyl)-1,4,7,10-tetraazacyclododecane-tetraacetic acid (C-DOTA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
14 Chopra, A., 177Lu-Labeled α-(5-isothiocyanato-2-methoxyphenyl)-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (MeO-DOTA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.